# IRDye 800CW-Human serum albumin

Chemical name: | IRDye 800CW-Human serum albumin
Abbreviated name: | HSA800
Synonym:
Agent category: | Polypeptide
Target: | Non-targeted
Target category: | Non-targeted, lymph node trapping
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | IRDye 800CW
Activation: | No
Studies: | - Rodents; - Non-primate non-rodent mammals; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about HSA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA800)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals or with probes in close proximity of the target in humans (4, 5). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment. It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon.

The sentinel lymph node (SLN) is considered to be the first lymph node to receive lymphatic flow from tumor sites and therefore, will contain metastatic tumor cells (6). SLN mapping has been used in diagnosis of metastasis of solid tumors (7). Radical lymph node dissection is performed in patients with malignant cells in the SLNs. Presently, SLN mapping is performed by a combination of radioactive tracer and blue dye, which require a radiologist. The current procedure is also time-consuming and requiring a steep learning curve. NIR quantum dots (QDs) has been studied in SLN mapping in small animals (4, 8). However, there are only limited studies of long-term toxicity of QDs in animals (9). IRDye CW800-CW is an indocyanine-type NIR fluorophore with peak absorption at 775 nm, and peak excitation emission at 796 nm. It provides a quantum yield of 9% with an extinction coefficient of 242,000 M^-1^cm^-1^. It has a molecular weight of 962 Da. Human serum albumin (HSA) has been successfully conjugated with IRDye 800CW to form IRDye 800CW-HSA (HSA800) for non-invasive NIR mapping of SLNs in small animals (10-12).

### Related Resource Links:

- Chapters in MICAD (HSA (http://www.ncbi.nlm.nih.gov/books?term=human%20serum%20albumin%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (HSA (http://www.ncbi.nlm.nih.gov/gene/213))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HSA (http://www.ncbi.nlm.nih.gov/omim/103600))
- Clinical trials (ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA800%20and%20conjugation)]

Commercially available IRDye 800CW-N-hydroxysuccinimide ester (LI-COR, Lincoln, NE) was used to conjugate HSA to form HSA800, which was purified by gel filtration chromatography to a purity of >98% (10). The molar ratio of IRDye 800CW to HSA was estimated to be 3.0 by spectrometric measurements. The hydrodynamic diameter of HSA800 was 7.4 nm with a molecular weight of 70 kDa. HSA800 has an extinction of coefficient of 237,000 M^-1^cm^-1^ and a quantum yield of 0.12 with a maximal excitation wavelength of 784 nm and a maximal emission wavelength of 802 nm in fetal bovine serum.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA800%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA800%20and%20rodentia)]

Parungo et al. (11) compared the accumulation of HSA800 (7.4 nm in diameter, 70 kDa) and QDs (15-20 nm, 400-800 kDa) in rats (n = 4) using an intraoperative NIR fluorescence imaging system. HSA800 (12 nmol/kg) and QDs (6.8 nmol/kg) injected into the peritoneal space of rats and fluorescence signals were monitored at 10-20 min, and 1, 4, and 24 h after injection. QDs drained to the celiac, superior mesenteric, and periportal lymph node groups within 20 min. This pattern remained the same at the later time points. HSA800 drained to these same lymph node groups at early time points but continued flowing to the mediastinal lymph nodes via the thoracic duct by I h. After bowel resection, both tracers were found in the thoracic, not abdominal lymph node groups. Additionally, HSA800 was no longer found in the thoracic duct but in the anterior chest wall and diaphragmatic lymphatics.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA800%20and%20pig)]

Ohnisbi et al. (10) performed SLN mapping of the intestine of pigs by injections with indocyanine green (ICG, 1.2 nm in diameter, 1 nmol), CW800-CA (1.3 nm, 1 nmol), ICG:HSA (7.3 nm, 1 nmol), HSA800 (7.4 nm, 1 nmol), QDs (15-20 nm, 0.04 nmol), and nanocoll800 (50 nm, 0.4 nmol). The best SLN retention was nanocoll800, followed by HSA800, ICG:HSA, and QDs. ICG and CW800-CA were not retained by the SLNs at all. A more rigorous evaluation of contrast agents was performed using the porcine lower limb by subcutaneous injections. HSA800 revealed ultra-fine lymphatic channels flowing to a single SLN. ICG failed to identify the SLN, whereas ICG:HSA showed barely the lymphatics, but not the SLNs.

Tanaka et al. (12) performed SLN mapping in Sinclair swine with spontaneous melanoma metastatic to regional lymph nodes. ICG:HSA (1 nmol), HSA800 (1 nmol) and QDs (0.01 nmol) were tested in six pigs with 4 separate primary melanomas by peri-tumoral, subcutaneous injections. All 12 injections identified the associated SLNs (proximal and distal) in the whole animal imaging. ICG:HSA exhibited slightly lower signal intensity than HSA800 and QDs. Pathological analysis confirmed the presence of metastatic tumor cells in proximal and distal SLNs but not in the nearby control lymph nodes.

Hutteman et al. (13) identified 32 of 32 (100%) SLNs in the colon and rectum of pigs (n = 4) under both in vivo and ex vivo conditions after injection of HSA800 (1 nmol).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA800%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA800%20and%20human)]

Hutteman et al. (13) injected HSA800 (50 nmol) submucosally circumferentially with a 5-mm margin around the tumors in 24 colorectal cancer patients. SLN mappings were performed in ex vivo tissue specimens. SLNs were identified in all 24 patients within 5 min after injection of HSA800 with nine patients showing lymph node metastases. In one patient out of 24 patients, a 3-mm mesenteric metastasis was found adjacent to a tumor-negative SLN (false-negative).

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Frangioni J.V., Kim S.W., Ohnishi S., Kim S., Bawendi M.G. (2007). Sentinel Lymph Node Mapping With Type-II Quantum Dots. Methods Mol Biol.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Morton D.L., Wen D.R., Wong J.H., Economou J.S., Cagle L.A., Storm F.K., Foshag L.J., Cochran A.J. (1992). Technical details of intraoperative lymphatic mapping for early stage melanoma. Arch Surg.
7 Schulze T., Bembenek A., Schlag P.M. (2004). Sentinel lymph node biopsy progress in surgical treatment of cancer. Langenbecks Arch Surg.
8 Zimmer J.P., Kim S.W., Ohnishi S., Tanaka E., Frangioni J.V., Bawendi M.G. (2006). Size series of small indium arsenide-zinc selenide core-shell nanocrystals and their application to in vivo imaging. J Am Chem Soc.
9 Pinaud F., Michalet X., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Iyer G., Weiss S. (2006). Advances in fluorescence imaging with quantum dot bio-probes. Biomaterials.
10 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
11 Parungo C.P., Soybel D.I., Colson Y.L., Kim S.W., Ohnishi S., DeGrand A.M., Laurence R.G., Soltesz E.G., Chen F.Y., Cohn L.H., Bawendi M.G., Frangioni J.V. (2007). Lymphatic drainage of the peritoneal space: a pattern dependent on bowel lymphatics. Ann Surg Oncol.
12 Tanaka E., Choi H.S., Fujii H., Bawendi M.G., Frangioni J.V. (2006). Image-guided oncologic surgery using invisible light: completed pre-clinical development for sentinel lymph node mapping. Ann Surg Oncol.
13 Hutteman M., Choi H.S., Mieog J.S., van der Vorst J.R., Ashitate Y., Kuppen P.J., van Groningen M.C., Lowik C.W., Smit V.T., van de Velde C.J., Frangioni J.V., Vahrmeijer A.L. (2011). Clinical translation of ex vivo sentinel lymph node mapping for colorectal cancer using invisible near-infrared fluorescence light. Ann Surg Oncol.